# [^177^Lu]-Labeled (S-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)

Chemical name: | [^177^Lu]-Labeled (S-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)
Abbreviated name: | [^177^Lu]C-DOTA-L8A4
Synonym:
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor variant III (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography; gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, functions, and signal transduction pathways of the various transmembrane epidermal growth factor receptors (EGFRs) are described elsewhere (1-3). The EGFRs are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (2, 3). Overexpression of the EGFR in tumors has been attributed to cellular amplification of the receptor gene, and this phenomenon may result in the production of a mutated receptor in the cell (2, 4). In addition, overexpression of the EGFR in tumors usually indicates a poor clinical prognosis for a cancer patient (4). The most common mutation observed in the receptor is the deletion of an extracellular domain segment of the EGFR, including the ligand-binding region, and this generates a variant known as EGFRvIII or de2-7 EGFR (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy was reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to a ligand due to the absence of a ligand-binding site, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain transformed cells, several anti-EGFR antibodies (http://google2.fda.gov/search?q=anti-EGFR+antibodies+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=6) that inhibit the activity of this receptor and small molecule drugs (http://google2.fda.gov/search?q=EGFR+Tyrosine+kinase+inhibitor&spell=1&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&ie=UTF-8&site=FDAgov&access=p) that block the downstream TK signaling pathway were developed and have been approved by the United States Food and Drug Administration for the treatment of certain cancers (2). The antibodies are designed to target the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which leads to downregulation of the EGFR on the cell surface. However, because EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). Hence, a monoclonal antibody (mAb), designated mAb806 and specifically targets the EGFRvIII, was generated and has been characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated ch806, was developed and evaluated in a phase I clinical trial involving patients with cancerous tumors that overexpressed the EGFRvIII. Results from this trial indicated that ch806 can be a suitable biotherapeutic agent to treat cancers (4). Various studies performed with mAb806 or ch806 are described in separate chapters of MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ch806%20AND%20micad%5Bbook%5D).

Studies are also in progress with another anti-EGFRvIII mAb, L8A4, to develop a radioimmunotherapeutic (RIT) agent for the treatment of cancer (9, 10). In a recent study, the use of acyclic ([(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A''-DTPA) and 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA) as well as the macrocyclic ligands (S)-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) and α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) was evaluated for the labeling of L8A4 with ^177^Lu, which was considered suitable to generate an RIT agent against cancer (10). The characteristics of the various ^177^Lu-labeled conjugates of L8A4 ([^177^Lu]-CHX-A''-DTPA-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4) were compared to the characteristics of L8A4 labeled with N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB-L8A4) under in vitro (9) and in vivo (10) conditions.

This chapter describes results obtained from the in vitro and the biodistribution studies performed with [^177^Lu]-C-DOTA-L8A4 in athymic mice bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors. Results obtained with [^125^I]SGMIB-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-CHX-A''-DTPA-L8A4 , and [^177^Lu]-MeO-DOTA-L8A4 are presented in separate chapters of MICAD (www.micad.nih.gov) (11-14).

### Other Sources of Information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=200086&source=NATURE&what=graphic&jpg=on) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Chapters on anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Other chapters on anti-EGFRvIII antibodies (http://www.ncbi.nlm.nih.gov/books/?term=EGFRvIII%20AND%20micad%5Bbook%5D) in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) with EGFRvIII as a target

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20L8A4%20antibody&cmd=DetailsSearch)]

The preparation, purification, characterization, the conjugation of L8A4 with C-DOTA, and radiolabeling of C-DOTA-L8A4 with ^177^Lu are discussed by Hens et al. (10). The production of [^125^I]SGMIB-L8A4 (labeled with ^125^I using N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB)) is also described by Hens et al. (10). The radiochemical yield (RCY) of [^177^Lu]C-DOTA-L8A4 was 73% (9). The RCY of [^125^I]SGMIB-L8A4 and the purity of the two labeled mAbs was not reported. The specific activity of [^177^Lu]-C-DOTA-L8A4 was reported to be 0.037 MBq/6.6 pmol (1.0 μCi/6.6 pmol) and that of [^125^I]SGMIB-L8A4 varied from 0.111–0.185 MBq/6.6 pmol (3–5 μCi/6.6 pmol) to 0.026–0.118 MBq/6.6 pmol (0.7–3.2 μCi/6.6 pmol). The two labeled mAbs were shown to elute as a single peak with L8A4 and had a similar retention time as the native mAb when analyzed with a size-exclusion column using high performance liquid chromatography. For C-DOTA-L8A4 each mAb molecule was determined to bear 3.1 moieties of C-DOTA (9, 10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20in%20vitro%20studies&cmd=DetailsSearch)]

Using a magnetic bead assay the immunoreactive fraction of [^177^Lu]-C-DOTA-L8A4 was determined to be 63% compared to between 60% to 71% for [^125^I]SGMIB-L8A4 (9). A cell internalization assay with U87MG.∆EGFR cells showed that internalization of [^177^Lu]-C-DOTA-L8A4 increased from ~10% at 1 h to ~35% at 24 h post exposure. In contrast internalization of the ^125^I-labeled mAb peaked to ~10% of the original cell-bound radioactivity at 1 h after exposure and was reduced to ~1% of the original value by 24 h after exposure.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^177^Lu]-C-DOTA-L8A4 was studied in athymic mice (n = 5 animals/group) bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors and compared it to that of [^125^I]SGMIB-L8A4 as described by Hens et al. (10). The different groups of animals were co-injected (route of injection not reported) with a mixture of the two labeled mAbs. The rodents were euthanized at 1, 4, and 8 days post injection (p.i.) of the labeled mAbs and all major organs were harvested from the animals. Radioactivity incorporated in the various organs was counted using a dual-channel automated gamma counter and the data was presented as percent of injected dose per gram tissue (% ID/g).

With [^177^Lu]-C-DOTA-L8A4 the amount of radioactivity in the blood was 10.95 ± 1.50% ID/g at 1 day p.i. and was reduced to 1.33 ± 1.60% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited an accumulation of between 4.21 ± 1.28% ID/g (lungs) and 13.00 ± 4.79% ID/g (liver); by 8 days p.i. the amount of label in all these organs decreased to between 0.72 ± 0.67% ID/g (lungs) and 5.39 ± 2.54% ID/g (Liver). The amount of tracer detected in the muscles was 1.32 ± 0.26% Id/g at 1 day p.i. and was reduced to 0.25 ± 0.16% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 23.52 ± 3.14% ID/g at 1 day p.i. and decreased to 7.47 ± 6.89% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 2, 5.5, 2, 80, and 5, respectively, at 1 day p.i. and approximately 1.2, 5, 1.2, 120 and 2, respectively at 8 days p.i.

With [^125^I]SGMIB-L8A4 the amount of radioactivity in the blood at 1 day p.i. was 18.78 ± 2.24% ID/g and decreased to 1.29 ± 0.87% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, and lungs exhibited accumulation between 5% and 7% ID/g and the amount of label in all these organs decreased to ~0.5% ID/g by 8 days p.i. The amount of tracer detected in the muscles and bones was ~1.5 and ~3.5% ID/g, respectively, at 1 day p.i.; by 8 days p.i., accumulation decreased to ~0.15% ID/g and ~0.33% ID/g, respectively, in these tissues. The tumor had a radioactivity accumulation of 21.64 ± 4.53% ID/g at 1 day p.i., which decreased to 2.86 ± 0.98% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 6, 8, 6, 60, and 10, respectively, at 1 day p.i. and approximately 7, 8, 7, 60 and 6, respectively, at 8 days p.i.

Table 1: Summary of tumor/normal tissue radioactivity uptake ratios for various organs obtained with [ ^ 125 ^ I]SGMIB-L8A4 and [ ^ 177 ^ Lu]C-DOTA-L8A4. Data obtained from Figure 5 in Hen et al. ( 10 ).

Conjugated mAb | Liver | | Kidney | | Spleen | | Brain | | Bone
Conjugated mAb | Time after labeled mAb injection
Conjugated mAb | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days
Conjugated mAb | Tumor-to-normal tissue ratio
[ ^ 125 ^ I]SGMIB-L8A4 | 6 | 7 | 8 | 8 | 6 | 7 | 60 | 60 | 10 | 6
[ ^ 177 ^ Lu]C-DOTA-L8A4 | 2 | 1.2 | 5.5 | 5 | 2 | 1.2 | 80 | 120 | 5 | 2

Based on the results presented in Table 1 [^125^I]SGMIB-L8A4 appeared to be superior to [^177^Lu]-C-DOTA-L8A4 for the detection of EGFRvIII overexpressing tumors in rodents because it had higher tumor-to-normal tissue ratios compared to the ^177^Lu-labeled mAb during the duration of the experiment (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by National Institutes of Health grants NS20023 and CA42324.

## References

1 Hasselbalch B., Lassen U., Poulsen H.S., Stockhausen M.T. (2010). Cetuximab insufficiently inhibits glioma cell growth due to persistent EGFR downstream signaling. Cancer Invest.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Hens M., Vaidyanathan G., Welsh P., Zalutsky M.R. (2009). Labeling internalizing anti-epidermal growth factor receptor variant III monoclonal antibody with (177)Lu: in vitro comparison of acyclic and macrocyclic ligands. Nucl Med Biol.
10 Hens M., Vaidyanathan G., Zhao X.G., Bigner D.D., Zalutsky M.R. (2010). Anti-EGFRvIII monoclonal antibody armed with 177Lu: in vivo comparison of macrocyclic and acyclic ligands. Nucl Med Biol.
11 Chopra, A., [125I]-Labeled monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., 177Lu-Labeled 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA)) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., 177Lu-Labeled (S-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
14 Chopra, A., 177Lu-Labeled α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.